# ^111^In/^125/131^I-Labeled anti-mucin-1 murine, chimeric or humanized antibody hPAM4

Chemical name: | ^111^In/^125/131^I-Labeled anti-mucin-1 murine, chimeric or humanized antibody hPAM4
Abbreviated name: | [^111^In/^125/131^I]-hPAM4
Synonym:
Agent Category: | Antibody
Target: | Mucin 1 (MUC1)
Target Category: | Antigen
Method of detection: | Single-photon emission tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In/^125/131^I
Activation: | No
Studies: | - Rodents; - Humans | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=hPAM4&cmd=DetailsSearch)]

Mucins (MUC) are a distinct class of transmembrane glycoproteins (designated as MUC1, MUC3A, MUC3B, MUC4, etc.) that are expressed primarily by the glandular and ductal cells of the epithelium in the human body and are known to modulate the tumorigenicity, progression, and pathogenesis of different cancers (1). The structure, physiological function, and process of promoting the development of malignancies by MUCs, particularly MUC1 and MUC4, are discussed in detail by Bafna et al. (1). MUC1 has been shown to be characteristically overexpressed by pancreatic adenocarcinoma (http://www.cancer.gov/dictionary?cdrid=46216) (PAC) cells and is not detectable in normal pancreatic ducts or other normal tissues, or during an incident of pancreatitis (2). Because it is detectable only in the serum of patients suffering from PAC, it was suggested recently that the MUC1 antigen can be used as a biomarker for the early detection this malignancy (3, 4).

The majority of individuals suffering from PAC do not survive for more than 1 year after diagnosis, and <1% of these patients live beyond 5 years (5). Although surgical resection of the cancer is a possible treatment for this disease, only 10%–25% of the patients are considered suitable for this treatment because, by the time that the neoplasm is detected, the malignancy has metastasized and the tumor load in the patient is too high to warrant surgery (5). Patients with nonresectable PAC are treated either with gemcitabine (http://www.cancer.gov/cancertopics/druginfo/gemcitabinehydrochloride) or radiotherapy; however, these treatments are not curative and only prolong survival and improve the quality of life of the patient (5). The detection of this invasive cancer at an early stage would facilitate proper staging of the disease, which could be followed either by surgical resection of the tumor or the initiation of a vigorous treatment regimen that could possibly improve patient prognosis (6).

More than a decade ago, a ^131^I-labeled murine monoclonal antibody, PAM4 ([^131^I]-mPAM4), directed against a mucin (later identified to be MUC1 (5)) was reported to detect human xenograft PAC tumors in mice with high specificity and, compared to controls, significantly extended the survival time of the animals when used for radiotherapy of the cancer (7-9). In a preliminary study, [^131^I]-PAM4 was demonstrated to detect the primary and the metastasized pancreatic carcinoma tumors in humans, and there was a low nonspecific uptake of the tracer in the liver, spleen, and bone marrow of the patients (10). In another study, a chimeric form of PAM4 (cPAM4) was labeled with ^125^I and ^111^In to obtain [^125^I]-cPAM4 and [^111^In]-cPAM4, respectively, and the biodistribution of these labeled mAbs was investigated in mice bearing human xenograft PAC tumors (11). Recently, Gulec et al. studied the biodistribution of ^111^In-labeled humanized PAM4 ( [^111^In]-hPAM4) in a phase I clinical trial (2).

### Other Sources of Information

Other anti-MUC1 antibody chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=MUC1%20AND%20micad%5Bbook%5D)

Chapters on radiolabeled antibodies in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=radiolabeled%20antibodies%20AND%20micad%5Bbook%5D)

Chimeric antibodies [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=chimeric%20antibody&cmd=DetailsSearch)]

Humanized antibodies [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=humanized%20antibodies&cmd=DetailsSearch)]

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/NM_002456.5) of human MUC1, transcript variant 1

MUC1 (http://www.ncbi.nlm.nih.gov/omim?term=MUC1) in Online Mendelian Inheritance in Man database (OMIM)

Information regarding MUC1 in Genetic Association Database (http://geneticassociationdb.nih.gov/cgi-bin/tableview.cgi?table=geneview&cond=GENE%20like%20'MUC1')

Gene information (http://www.ncbi.nlm.nih.gov/omim?Db=gene&DbFrom=omim&Cmd=Link&LinkName=omim_gene&LinkReadableName=Gene&IdsFromResult=158340) of MUC1 (Gene ID: 4582)

MUC1 related Clinical trials (http://clinicaltrials.gov/ct2/results?term=MUC1)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Radiolabeled-PAM4%20synthesis&cmd=DetailsSearch)]

The mPAM4 (8), cPAM4 (11), and hPAM4 (2) used in the different investigations were obtained from a commercial source.

mPAM4 was labeled with ^131^I using the chloramine-T method, and the specific activity (SA) of the labeled antibody was reported to be 259–444 kBq/μg (7–12 μCi/μg) (7). The [^131^I]-mPAM4 preparation contained <3% free ^131^I and no aggregates as determined with thin-layer chromatography (TLC). Gold et al. labeled mPAM4 with ^131^I using the Iodo-Gen procedure (5). The labeling efficiency of this method was reported to be 90%; the SA of the labeled mAb was 370–555 MBq/mg (10–15 mCi/mg), and the final preparation contained <5% unbound radioactivity as determined with high-performance liquid chromatography (HPLC) (5).

cPAM4 was labeled with ^125^I using the chloramine-T procedure as described above (11). The labeled mAb had a SA of 365.6–455 kBq/μg (9.88–12.3 μCi/μg) and contained <5% unbound ^125^I and <8% aggregates.

cPAM4 was labeled with ^111^In after conjugation of the mAb to 1,4,7,10-tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid (DOTA) (11), and the DOTA:cPAM4 ratio of the conjugate was reported in another publication to be 3.3 (12). The SA of [^111^In]-cPAM4 was reported to vary from 200 kBq/μg (5.41 μCi/μg) to 48.1–133.2 MBq/mg (1.3–3.6 mCi/mg) and contained <1.7% unbound radionuclides and <1% aggregates (5, 11, 12).

The biodistribution and tumor targeting of [^111^In]-hPAM4 was investigated in patients suffering from pancreatic cancer in a phase I clinical trial (2). Although the [^111^In]-hPAM4 preparation used in the clinical investigation was reported to contain <10% free radionuclide as determined with instant TLC, the SA of the labeled antibody was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=PAM4%20in%20vitro&cmd=DetailsSearch)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=PAM4%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^131^I]-mPAM4 was investigated in nu/nu mice bearing xenograft orthotopic CaPan-1 cell (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-79&Template=cellBiology) tumors as described by Alisauskus et al. (7). The mice (n = 5–8 animals/group) were injected with 25 μCi [^131^I]-mPAM4 (route of injection was not reported) and euthanized at various time points from 1 d to 14 d postinjection (p.i.). All major organs were removed from the animals, and the amount of accumulated radioactivity in the tissues was determined. Data obtained from this study were presented as the percentage of injected dose per gram tissue (% ID/g). The amount of radioactivity in the tumor was shown to decrease steadily from ~15% ID/g at day 1 p.i. to ~4% ID/g at day 14 p.i. In all other organs, the accumulation of radioactivity was between ~2% ID/g (kidneys) and ~5% ID/g (both spleen and blood) on day 1 p.i., and accumulation reduced to <1% ID/g by day 14 p.i. in all the organs. Ex vivo microautoradigraphy of 5-μm tumor sections showed that the radioactivity was confined within the tumors and no tracer was detected in the surrounding normal tissues (7). No blocking studies were reported.

In another study, Cardillo et al. investigated the biodistribution of [^125^I]-cPAM4 in athymic mice bearing CaPan-1 cell tumors (11). The biodistribution pattern of the ^125^I-labeled chimeric mAb was shown to be similar to that of [^131^I]-mPAM4 as described above.

Gold et al. studied the biodistribution of [^111^In]-cPAM4 (used as a surrogate for immunotherapeutic ^90^Y-labeled cPAM4) in athymic mice bearing similarly sized CaPan-1 cell tumors (5). The animals (n = at least 8 mice/group) were injected with 25 μCi labeled cPAM4 for a total of 25 μg protein/animal, and the preparation also contained the unlabeled chimeric antibody. The mice were euthanized on days 1, 4 and 7 p.i., and all major organs were removed to determine the amount of accumulated radioactivity. The uptake of radioactivity by the tumor was ~25% ID/g on day 1 p.i., increased to ~40% ID/g by day 4 p.i., and decreased to ~25% ID/g on day 7 p.i. During the same period, the accumulation of the tracer in all major organs was between ~2% ID/g (normal pancreas) and ~10% ID/g (blood) on day 1 p.i., and between 2% ID/g (blood) and ~7% ID/g (liver) on day 7 p.i. The amount of tracer in the liver remained constant during the entire period of the study, indicating that the radioactivity was excreted primarily through the hepatobiliary route. The estimated potential radiation dose received by the tumor, the tumor/blood radiation ratio, and the maximum tolerated dose of [^90^Y]-cPAM4 for the animals were described elsewhere (5). Other investigators reported a similar biodistribution pattern for [^111^In]-cPAM4 in athymic nu/nu mice bearing CaPan-1 cell tumors (11).

In another study, mice bearing subcutaneous CaPan-1 cell tumors were injected with [^111^In]-cPAM4, and whole-body immunoscintigraphic images were acquired from the animals (n = 2 mice) at various time points as described by Cardillo et al. (12). At 24 h p.i., high background levels of the tracer were observed in the thoracic and abdominal areas of the animals, and the tumors on the animals became visible clearly only at 48 h p.i., indicating a slow clearance of radioactivity from the mice (12). In another part of the same study (n = 14 animals), the tumor/blood, tumor/liver, tumor/kidney, and tumor/normal pancreas radioactivity uptake ratios were reported to be 2.4 ± 1.0, 3.5 ± 1.6, 5.9 ± 1.3, and 18.6 ± 8.2, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=PAM4%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=PAM4%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=PAM4%20Human%20Studies&cmd=DetailsSearch)]

Two patients with histologically confirmed metastatic pancreatic cancer were injected with [^131^I]-mPAM4; one patient received 270 MBq (7.3 mCi) [^131^I]-mPAM4 in a protein dose of 0.6 mg, and the other patient received 315 MBq (8.5 mCi) [^131^I]-mPAM4 in a protein dose of 0.6 mg (5). Blood samples taken from the two patients showed that the clearance of radioactivity from this tissue was biexponential. The circulating half-life of the tracer in the early component of the curve was 1.9 h in the patient with the smaller dose and 4.6 h in the patient with the larger dose; in the late component the half-life values were 28.6 h and 39.2 h, respectively. HPLC analysis of the plasma obtained from these patients at 24 h p.i. showed the presence of 66%–78% ^131^I in the small molecular weight fraction, indicating that mPAM4 was catabolized in the blood within 24 h p.i. Scintigraphy was performed on a patient injected with [^131^I]-mPAM4 (the patient had previously undergone chemotherapy and radiotherapy for the treatment of PAC), and clear uptake of the tracer was observed in tumors on the left hepatic lobe and in the mid-abdomen area of the patient (5). Similarly, tumors were also detected in posterior and anterior planar images acquired from a second patient injected with the radioiodinated mAb (5). From this study, the investigators concluded that mPAM4 specifically targeted pancreatic cancer tumors in the patients.

In a phase I clinical study to evaluate the efficacy of [^90^Y]-hPAM4 for the treatment of PAC, 21 patients (4 patients with stage III, locally advanced disease; 17 patients with stage IV metastatic disease) were administered a slow intravenous injection of [^111^In]-hPAM4 to investigate the biodistribution of the tracer (a surrogate for the ^90^Y-labeled homolog) in the individuals (2). The patients received 3–5 mCi of the label, and the total protein content of each dose, including the unlabeled hPAM4, was 10 mg (for 6 patients) and 100 mg (for 16 patients). Starting at 4 h p.i., repeat whole-body planar scintigraphic images were acquired from the patients over 7 days. Pancreatic tumors were clearly visible at 24 h p.i. (only a representative image was presented (2)), and the visibility was progressively prominent on the subsequent images. From a review of the various images obtained from this study, the investigators concluded there was no qualitative difference was apparent in the biodistribution of [^111^In]-hPAM4 at the two doses (10 and 100 mg total hPAM4), the humanized mAb showed a normal biodistribution in the patients suffering from PAC and was suitable for the scintigraphic visualization of PAC tumors in humans (2).

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Studies described in this chapter were supported in part by grants CA39841, CA43218, and CA54425 from the National Institutes of Health.

## References

1 Bafna S., Kaur S., Batra S.K. (2010). Membrane-bound mucins: the mechanistic basis for alterations in the growth and survival of cancer cells. Oncogene.
2 Gulec S.A., Cohen S.J., Pennington K.L., Zuckier L.S., Hauke R.J., Horne H., Wegener W.A., Teoh N., Gold D.V., Sharkey R.M., Goldenberg D.M. (2011). Treatment of Advanced Pancreatic Carcinoma with 90Y-Clivatuzumab Tetraxetan: A Phase I Single-Dose Escalation Trial. Clin Cancer Res.
3 Gold D.V., Karanjawala Z., Modrak D.E., Goldenberg D.M., Hruban R.H. (2007). PAM4-reactive MUC1 is a biomarker for early pancreatic adenocarcinoma. Clin Cancer Res.
4 Gold D.V., Modrak D.E., Ying Z., Cardillo T.M., Sharkey R.M., Goldenberg D.M. (2006). New MUC1 serum immunoassay differentiates pancreatic cancer from pancreatitis. J Clin Oncol.
5 Gold D.V., Cardillo T., Goldenberg D.M., Sharkey R.M. (2001). Localization of pancreatic cancer with radiolabeled monoclonal antibody PAM4. Crit Rev Oncol Hematol.
6 Gold D.V., Goggins M., Modrak D.E., Newsome G., Liu M., Shi C., Hruban R.H., Goldenberg D.M. (2010). Detection of early-stage pancreatic adenocarcinoma. Cancer Epidemiol Biomarkers Prev.
7 Alisauskus R., Wong G.Y., Gold D.V. (1995). Initial studies of monoclonal antibody PAM4 targeting to xenografted orthotopic pancreatic cancer. Cancer Res.
8 Gold D.V., Alisauskas R., Sharkey R.M. (1995). Targeting of xenografted pancreatic cancer with a new monoclonal antibody, PAM4. Cancer Res.
9 Gold D.V., Cardillo T., Vardi Y., Blumenthal R. (1997). Radioimmunotherapy of experimental pancreatic cancer with 131I-labeled monoclonal antibody PAM4. Int J Cancer.
10 Mariani G., Molea N., Bacciardi D., Boggi U., Fornaciari G., Campani D., Salvadori P.A., Giulianotti P.C., Mosca F., Gold D.V., et al. (1995). Initial tumor targeting, biodistribution, and pharmacokinetic evaluation of the monoclonal antibody PAM4 in patients with pancreatic cancer. Cancer Res.
11 Cardillo T.M., Ying Z., Gold D.V. (2001). Therapeutic advantage of (90)yttrium- versus (131)iodine-labeled PAM4 antibody in experimental pancreatic cancer. Clin Cancer Res.
12 Cardillo T.M., Karacay H., Goldenberg D.M., Yeldell D., Chang C.H., Modrak D.E., Sharkey R.M., Gold D.V. (2004). Improved targeting of pancreatic cancer: experimental studies of a new bispecific antibody, pretargeting enhancement system for immunoscintigraphy. Clin Cancer Res.